# 2-[2-([O-^11^C]Tolyl)ethyl]-4,5-dihydro-1H-imidazole

Chemical name: | 2-[2-([O-^11^C]Tolyl)ethyl]-4,5-dihydro-1H-imidazole
Abbreviated name: | [^11^C]TEIMD
Synonym:
Agent category: | Compound
Target: | I_2_-imidazoline receptor (I_2_R)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TEIMD)]

Two major imidazoline binding sites (I_1_R and I_2_R) have been identified (1, 2). The I_1_R and I_2_R exhibit high affinities for clonidine and idazoxan, respectively. Clonidine and its analogs mediate effects independent of α_2_-adrenoceptor at the IR receptors. IR receptors are widely distributed in the central and peripheral nervous systems and in various organs such as the pancreas, liver, kidney, lung, and heart (3-6). I_1_R is associated with hypertension (7), whereas I_2_R is associated with depression (8), Alzheimer’s disease (9), Parkinson’s disease (10), Huntington’s disease (10), and glial cell tumors (11). High densities of I_2_R have been observed in the arcuate nucleus, interpeduncular nucleus, pineal gland, and ventricles in human brain (12). The I_2_R gene has not been identified. Tesson et al. (13) showed that I_2_R is localized to the mitochondrial outer membrane of the human and rabbit liver. Gentili et al. (14) showed that 2-[2-(O-tolyl)ethyl]-4,5-dihydro-1H-imidazole (TEIMD) has a high and selective affinity for I_2_R. 2-[2-([o-^11^C]Tolyl)ethyl]-4,5-dihydro-1H-imidazole ([^11^C]TEIMD) was evaluated as a PET probe for imaging of I_2_R in the peripheral tissues (15).

### Related Resource Links:

- Chapters in MICAD (Imidazoline receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Imidazoline%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (I_1_R (http://www.ncbi.nlm.nih.gov/gene/11188), α_2_-adrenoceptors (http://www.ncbi.nlm.nih.gov/gene?term=alpha%20adrenoceptor%20human))
- Articles in OMIM (I_1_R (http://omim.org/entry/601174), α_2_-adrenoceptors (http://omim.org/search?index=entry&start=1&limit=10&search=alpha-2-adrenergic+receptor&sort=score+desc+%2C+prefix_sort+desc&sort=score+desc+%2C+prefix_sort+desc))
- Clinical trials (Clonidine (http://www.clinicaltrials.gov/ct2/results?term=clonidine))
- Drug information in FDA (Clonidine (http://google2.fda.gov/search?q=clonidine&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TEIMD%20and%20synthesis)]

[^11^C]TEIMD was synthesized remotely via a reaction of [^11^C]methyl iodine (produced from [^11^C]CO_2_) with the tributylsannyl precursor in the presence of tris(dibenzylideneacetone)dipalladium(0), CuCl_2_, potassium carbonate and tri(O-tolyl)phosphine in dimethylformamide at 80°C for 5 min (14). [^11^C]TEIMD was purified with high-performance liquid chromatography with a radiochemical yield of 13.6 ± 4.4% (n = 3) from [^11^C]CO_2_ at end of bombardment (EOB). The radiochemical purity was >95%, and the specific activity was 79 ± 40 GBq/μmol (2.1 ± 1.1 Ci/μmol) at end of synthesis. Total time of synthesis was 30 min from EOB.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TEIMD%20and%20in%20vitro)]

On the basis of in vitro competition binding studies, Gentili et al. (14) reported inhibition constant (K_i_) values for TEIMD of 1.7 nM for I_2_R, >2,000 nM for I_1_R and 560 nM for α_2_-adrenoceptor. cLogD (pH 7.4) value for TEIMD was 1.73.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TEIMD%20and%20rodentia)]

Ex vivo biodistribution of 9.1-13.4 MBq (0.25-0.36 mCi) [^11^C]TEIMD was studied in normal mice (n = 4/group) at 5, 15, 30 and 60 min after injection (15). The tissue with the highest accumulation at 5 min after injection was the liver (10% injected dose/gram (ID/g)), followed by the lung (6% ID/g), kidney (5% ID/g), small intestine (5% ID/g), pancreas (5% ID/g), heart (3% ID/g), spleen (2% ID/g), muscle (2% ID/g), blood (1% ID/g), and brain (0.1% ID/g). All these tissues showed moderate to rapid washout. Co-injection of I_1_R inhibitor moxonidine (1 mg/kg) and I_2_R inhibitor BU224 (1 mg/kg) resulted with little inhibition of radioactivity in the liver and pancreas at 30 min after injection. Hence, [^11^C]TEIMD is not suitable as a PET agent for imaging I_2_R in the peripheral tissues.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TEIMD%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TEIMD%20and%20primate)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TEIMD%20and%20human)]

No publications are currently available.

## References

1 Michel M.C., Ernsberger P. (1992). Keeping an eye on the I site: imidazoline-preferring receptors. Trends Pharmacol Sci.
2 Hamilton C.A. (1995). Imidazoline receptors, subclassification, and drug-induced regulation. Ann N Y Acad Sci.
3 El-Ayoubi R., Gutkowska J., Regunathan S., Mukaddam-Daher S. (2002). Imidazoline receptors in the heart: characterization, distribution, and regulation. J Cardiovasc Pharmacol.
4 Ernsberger P., Graves M.E., Graff L.M., Zakieh N., Nguyen P., Collins L.A., Westbrooks K.L., Johnson G.G. (1995). I1-imidazoline receptors. Definition, characterization, distribution, and transmembrane signaling. Ann N Y Acad Sci.
5 Ruggiero D.A., Regunathan S., Wang H., Milner T.A., Reis D.J. (1995). Distribution of imidazoline receptor binding protein in the central nervous system. Ann N Y Acad Sci.
6 Lanier S.M., Ivkovic B., Singh I., Neumeyer J.L., Bakthavachalam V. (1993). Visualization of multiple imidazoline/guanidinium-receptive sites. J Biol Chem.
7 Nikolic, K. and D. Agbaba, Imidazoline Antihypertensive Drugs: Selective I(1) -Imidazoline Receptors Activation. Cardiovasc Ther, 2011
8 Piletz J.E., Zhu H., Ordway G., Stockmeier C., Dilly G., Reis D., Halaris A. (2000). Imidazoline receptor proteins are decreased in the hippocampus of individuals with major depression. Biol Psychiatry.
9 Garcia-Sevilla J.A., Escriba P.V., Walzer C., Bouras C., Guimon J. (1998). Imidazoline receptor proteins in brains of patients with Alzheimer's disease. Neurosci Lett.
10 Reynolds G.P., Boulton R.M., Pearson S.J., Hudson A.L., Nutt D.J. (1996). Imidazoline binding sites in Huntington's and Parkinson's disease putamen. Eur J Pharmacol.
11 Martin-Gomez J.I., Ruiz J., Callado L.F., Garibi J.M., Aguinaco L., Barturen F., Javier Meana J. (1996). Increased density of I2-imidazoline receptors in human glioblastomas. Neuroreport.
12 De Vos H., Bricca G., De Keyser J., De Backer J.P., Bousquet P., Vauquelin G. (1994). Imidazoline receptors, non-adrenergic idazoxan binding sites and alpha 2-adrenoceptors in the human central nervous system. Neuroscience.
13 Tesson F., Prip-Buus C., Lemoine A., Pegorier J.P., Parini A. (1991). Subcellular distribution of imidazoline-guanidinium-receptive sites in human and rabbit liver. Major localization to the mitochondrial outer membrane. J Biol Chem.
14 Gentili F., Cardinaletti C., Vesprini C., Ghelfi F., Farande A., Giannella M., Piergentili A., Quaglia W., Mattioli L., Perfumi M., Hudson A., Pigini M. (2008). Novel ligands rationally designed for characterizing I2-imidazoline binding sites nature and functions. J Med Chem.
15 Kawamura K., Yui J., Konno F., Yamasaki T., Hatori A., Wakizaka H., Fujinaga M., Kumata K., Yoshida Y., Ogawa M., Nengaki N., Yanamoto K., Fukumura T., Zhang M.R. (2012). Synthesis and evaluation of PET probes for the imaging of I2 imidazoline receptors in peripheral tissues. Nucl Med Biol.